# 2-tert-Butyl-4-chloro-5-[4-(2-[^18^F]fluoroethoxymethyl)-benzyloxy]-2H-pyridazin-3-one

Chemical name: | 2-tert-Butyl-4-chloro-5-[4-(2-[^18^F]fluoroethoxymethyl)-benzyloxy]-2H-pyridazin-3-one
Abbreviated name: | BMS-747158-02
Synonym: | [^18^F]BMS-747158-01, [^18^F]Flurpiridaz
Agent category: | Compound
Target: | Mitochondrial complex I (MCI)
Target category: | Enzyme
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents; - Non-primate non-rodent mammals; - Non-human primates; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=BMS-747158-02)]

Lipophilic cations are capable of passing through biological membranes by passive diffusion into the cytoplasm and mitochondria of cells in response to large negative plasma and mitochondrial membrane potentials. ^99m^Tc-2-Methoxyisobutylisonitrile (^99m^Tc-MIBI) and ^99m^Tc-tetrofosmin are delocalized lipophilic cations, which are rapidly taken up into cells driven by membrane potential (1-4). They are used as agents for myocardial-perfusion single-photon emission computed tomography and tumor imaging. However, the high accumulation of technetium tracers in the lung and liver may interfere with the detection of flow abnormalities in the myocardium. More recently, positron emission tomography (PET) imaging has emerged as an alternative approach for the evaluation of myocardial blood flow by use of positron-emitting radionuclides (e.g., ^82^RbCl, ^13^NH_3_, and H_2_^15^O). However, the majority of these radiotracers exhibit short physical half-lives (<20 min), and they cannot be distributed from a central radiopharmacy. Lipophilic cations, such as ^11^C-labeled triphenylmethylphosphonium ([^11^C]TPMP) (5) and 4-[^18^F]fluorobenzyl-triphenylphosphonium ([^18^F]FBnTP) have been investigated as PET agents for myocardial and tumor imaging (6).

Mitochondrial complex I (MCI) of the mammalian electron transfer chain is composed of at least 43 protein subunits, of which seven are encoded by mitochondrial DNA (7). MCI catalyzes the transfer of electrons from NADH to ubiquinone and translocates protons from the mitochondrial matrix to the intermembrane space to generate ATP and thereby the energy supply of the cell. MCI may also play direct roles in the mitochondrial permeability transition and in cell death pathways. Myocardium has a high mitochondrial content because of high energy use. 2-tert-Butyl-4-chloro-5-[4-(2-fluoroethoxymethyl)-benzyloxy]-2H-pyridazin-3-one (BMS-747158-01), an analog of the MCI inhibitor pyridaben (8), is found to be a potent MCI inhibitor with a hydrophobic heterocyclic pyridazinone moiety (9). 2-tert-Butyl-4-chloro-5-[4-(2-[^18^F]fluoroethoxymethyl)-benzyloxy]-2H-pyridazin-3-one (BMS-747158-02) has been synthesized and studied as a PET agent used to image myocardium.

### Related Resource Links:

- Chapters in MICAD (MCI (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=Mitochondrial%20complex+AND+micad%5Bbook%5D))
- Gene information in NCBI (MCI (http://www.ncbi.nlm.nih.gov/gene/291))
- Articles in Online Mendelian Inheritance in Man (OMIM) (MCI (http://www.ncbi.nlm.nih.gov/entrez/dispomim.cgi?id=252010))
- Clinical trials (MCI (http://www.clinicaltrials.gov/ct2/results?term=Mitochondrial+complex+I+), [^18^F]Flurpiridaz (http://www.clinicaltrials.gov/ct2/show/NCT01347710?term=Flurpiridaz&rank=1))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=BMS-747158-02+synthesis)]

BMS-747158-02 was prepared by fluorination of the toluene sulfonate ester precursor followed by purification with high-performance liquid chromatography (9). Average radiochemical yield (decay-corrected) was ~25%. Radiochemical purity was >95% with specific activities of 57–204 TBq/mmol (1,550–5,500 Ci/mmol) at the end of synthesis.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%20BMS-747158-02%20and%20in%20vitro)]

Yalamanchili et al. (9) reported that BMS-747158-01 inhibited MCI NADH oxidation in bovine heart submitochondrial particles with a 50% inhibition concentration value of 16.6 ± 3 nM, which was comparable to the reference inhibitors of MCI (i.e., rotenone (18.2 ± 6.7 nM), pyridaben (19.8 ± 2.6 nM), and deguelin (23.1 ± 1.5 nM)). BMS-747158-02 had a high uptake in neonatal rat cardiomyocytes with 10.3 ± 0.7% of the incubated dose at 60 min. Rotenone (200 nM) and deguelin (200 nM) inhibited tracer accumulation in cardiomyocytes by 91 ± 2% and 89 ± 3%, respectively. The uptake of BMS-747158-02 was rapid with a half-maximal uptake time of ~0.5 min, whereas its retention was excellent with a half-maximal washout for efflux of >120 min.

Yu et al. (10) measured heart uptake in an isolated rabbit heart model at flow rates of 1.66–5.06 ml/min per g wet left ventricular weight. The net BMS-747158-02 heart uptake increased proportionally (0.93 ± 0.15 to 2.44 ± 0.40 ml/min per g) and to a greater extent than that of ^201^thallium (0.76 ± 0.02 to 1.11 ± 0.02 ml/min per g) or ^99m^Tc-sestamibi (0.49 ± 0.03 to 0.77 ± 0.08 ml/min per g).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%20BMS-747158-02%20and%20rodentia)]

Yalamanchili et al. (9) performed biodistribution studies of BMS-747158-02 in mice. BMS-747158-02 accumulated mainly in the heart (9.5 ± 0.5% injected dose per gram (ID/g)) at 60 min after injection with heart/lung and heart/liver ratios of 14.1 ± 2.5 and 8.3 ± 0.5, respectively. The accumulation in the kidney was ~4% ID/g with low blood radioactivity (~0.3% ID/g). PET imaging showed that BMS-747158-02 accumulated mainly in the heart and kidney. Good myocardial images were observed at 5–15 min after injection with little interference from the lung by 55–65 min. No blocking experiment was performed.

Yu et al. (10) performed a biodistribution study in rats, which showed that 0.56 MBq (0.015 mCi) BMS-747158-02 had substantially higher myocardial uptake than 3.7 mBq (0.1 mCi) ^99m^Tc-sestamibi at 15 minutes (3.5 ± 0.3% ID/g versus 1.9 ± 0.1% ID/g) and 120 minutes (3.2 ± 0.4% ID/g versus 1.8 ± 0.0% ID/g) after injection. Heart/lung and heart/liver uptake ratios at 60 minutes were also higher for BMS-747158-02 (12.7 ± 1.4 and 3.7 ± 0.2, respectively) than ^99m^Tc-sestamibi (5.9 ± 0.5 and 2.4 ± 0.4, respectively). PET imaging with BMS-747158-02 showed a clear and sustained cardiac uptake in rats (n = 4) because of the minimal lung accumulation and rapid liver clearance at 55–65 min. Myocardial infarct areas created by either permanent left coronary ligation or reperfusion after ligation in rats were both clearly identified on PET cardiac images of BMS-747158-02 and had good agreement with in vitro triphenyltetrazolium chloride staining for cell viability.

Hiquchi et al. (11) performed PET imaging of myocardial BMS-747158-02 distribution in healthy rats (n = 7), rats with transient (3-min) left coronary artery occlusion (n = 11), and rats with permanent left coronary occlusion (n = 11). Normal hearts demonstrated intense and almost homogeneous tracer uptake throughout the left ventricle for more than 2 h. During permanent coronary occlusion, PET imaging demonstrated perfusion defects, which remained unchanged (37.6% ± 8.8%, 37.4% ± 10.2%, and 36.2% ± 9.8% left ventricle at 15, 45, and 115 min after tracer injection, respectively). After transient ischemia, the induced defect size decreased significantly after reperfusion (16.2% ± 9.3%, 6.0% ± 6.5%, and 1.4% ± 1.3% left ventricle) (P < 0.01). Tracer reinjection after transient ischemia resulted in normalization of the induced defect.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=BMS-747158-02+and+(dog+or+pig+or+sheep+or+rabbit))]

PET imaging with BMS-747158-02 showed a clear and sustained cardiac uptake in three rabbits, with minimal lung interference and rapid liver clearance at 55–65 min (10).

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%20BMS-747158-02%20and%20%28primate%20not%20human%29)]

PET imaging with BMS-747158-02 showed a clear and sustained cardiac uptake in five monkeys (Rhesus macaque), with minimal lung interference and rapid liver clearance at 55–65 min (10). The heart/liver ratio was 1.3 ± 0.3 at 5 min and 2.5 ± 0.5 at 60 min.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%20BMS-747158-02%20and%20human)]

Maddahi et al. (12) estimated the human dosimetry of BMS-747158-02 in 13 healthy subjects after injection of 170-244 MBq (4.6-6.6 mCi) of BMS747158. The organ receiving the highest radiation dose was the kidney at 0.066 mSv/MBq (0.24 rem/mCi), followed by the heart wall at 0.048 mSv/MBq (0.18 rem/mCi). The mean effective dose was 0.019 mSv/MBq (0.072 rem/mCi) with mean urinary excretion of 4.83% ID.

## References

1 Chernoff D.M., Strichartz G.R., Piwnica-Worms D. (1993). Membrane potential determination in large unilamellar vesicles with hexakis(2-methoxyisobutylisonitrile)technetium(I). Biochim Biophys Acta.
2 Chiu M.L., Kronauge J.F., Piwnica-Worms D. (1990). Effect of mitochondrial and plasma membrane potentials on accumulation of hexakis (2-methoxyisobutylisonitrile) technetium(I) in cultured mouse fibroblasts. J Nucl Med.
3 Molteni S.N., Seregni E., Botti C., Martinetti A., Ferrari L., Crippa F., Bombardieri E. (1999). The breast cancer cell line MCF7 as a model of 99mTc-SestaMIBI, 99mTc-tetrofosmin and 99mTc-Medronate incorporation. Anticancer Res.
4 Younes A., Songadele J.A., Maublant J., Platts E., Pickett R., Veyre A. (1995). Mechanism of uptake of technetium-tetrofosmin. II: Uptake into isolated adult rat heart mitochondria. J Nucl Cardiol.
5 Krause B.J., Szabo Z., Becker L.C., Dannals R.F., Scheffel U., Seki C., Ravert H.T., Dipaola A.F., Wagner H.N. (1994). Myocardial perfusion with [11C]methyl triphenyl phosphonium: measurements of the extraction fraction and myocardial uptake. J Nucl Biol Med.
6 Madar I., Ravert H.T., Du Y., Hilton J., Volokh L., Dannals R.F., Frost J.J., Hare J.M. (2006). Characterization of Uptake of the New PET Imaging Compound 18F-Fluorobenzyl Triphenyl Phosphonium in Dog Myocardium. J Nucl Med.
7 Lenaz G., Fato R., Genova M.L., Bergamini C., Bianchi C., Biondi A. (2006). Mitochondrial Complex I: structural and functional aspects. Biochim Biophys Acta.
8 Degli Esposti M. (1998). Inhibitors of NADH-ubiquinone reductase: an overview. Biochim Biophys Acta.
9 Yalamanchili P., Wexler E., Hayes M., Yu M., Bozek J., Kagan M., Radeke H.S., Azure M., Purohit A., Casebier D.S., Robinson S.P. (2007). Mechanism of uptake and retention of F-18 BMS-747158-02 in cardiomyocytes: a novel PET myocardial imaging agent. J Nucl Cardiol.
10 Yu M., Guaraldi M.T., Mistry M., Kagan M., McDonald J.L., Drew K., Radeke H., Azure M., Purohit A., Casebier D.S., Robinson S.P. (2007). BMS-747158-02: a novel PET myocardial perfusion imaging agent. J Nucl Cardiol.
11 Higuchi T., Nekolla S.G., Huisman M.M., Reder S., Poethko T., Yu M., Wester H.J., Casebier D.S., Robinson S.P., Botnar R.M., Schwaiger M. (2008). A new 18F-labeled myocardial PET tracer: myocardial uptake after permanent and transient coronary occlusion in rats. J Nucl Med.
12 Maddahi J., Czernin J., Lazewatsky J., Huang S.C., Dahlbom M., Schelbert H., Sparks R., Ehlgen A., Crane P., Zhu Q., Devine M., Phelps M. (2011). Phase I, first-in-human study of BMS747158, a novel 18F-labeled tracer for myocardial perfusion PET: dosimetry, biodistribution, safety, and imaging characteristics after a single injection at rest. J Nucl Med.